# ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetracetic acid-Glu{PEG_4_-Glu[cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)}-{PEG_4_-Glu[cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)} (PEG_4_ = 15 amino-4,7,10,13-tetraoxapentadecanoic acid)

Chemical name: | ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetracetic acid-Glu{PEG_4_-Glu[cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)}-{PEG_4_-Glu[cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)} (PEG_4_ = 15 amino-4,7,10,13-tetraoxapentadecanoic acid) | [image]
Abbreviated name: | ^111^In(DOTA-6P-RGD_4_) | [image]
Synonym: | ^111^In-DOTA-E{PEG_4_-E[PEG_4_-c(RGDfK)]_2_}_2_ | [image]
Agent Category: | Peptides | [image]
Target: | Integrin alphavbeta3 (α_v_β_3_) | [image]
Target Category: | Receptors | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) or planar imaging | [image]
Source of signal / contrast: | ^111^In | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of ^111^In(DOTA-6P-RGD_4_) by Shi et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Integrin%20%u03B1v%u03B23%20and%20imaging)]

The ^111^In-labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetracetic acid (DOTA)-Glu{PEG_4_-Glu[cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)}-{PEG_4_-Glu[cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)]-cyclo(Lys(PEG_4_)-Arg-Gly-Asp-D-Phe)}, abbreviated as ^111^In(DOTA-6P-RGD_4_) or ^111^In-DOTA-E{PEG_4_-E[PEG_4_-c(RGDfK)]_2_}_2_, was synthesized by Shi et al. as an agent for molecular imaging of tumor angiogenesis by targeting integrin alphavbeta3 (α_v_β_3_) (1). Here, P = PEG_4_ = 15 amino-4,710,13-tetraoxapentadecanoic acid = a linker between two c(RGDfK) motifs; c(RGDfK) = cyclo(Lys-Arg-Gly-Asp-D-Phe); RGD_4_ = four motifs of c(RGDfK); and E = Glu.

Integrin α_v_β_3_ is a receptor that is overexpressed on the activated endothelial cells of tumors (2). Because the integrin α_v_β_3_ binds with extracellular matrix proteins (e.g., vitronectin, fibronectin) through the exposed Arg-Gly-Asp tripeptide sequence, RGD-containing peptides have been intensively studied in the past decade as a vector for imaging α_v_β_3_ expression (3, 4). Although significant progress has been made, improving the binding affinity and pharmacokinetics of RGD peptides remains the major consideration in the design of agents, and various strategies have been developed for this improvement, such as the use of RGD multimers, the introduction of sugar amino acids or D-amino acids into the RGD peptides, and the conjugation of the RGD peptides with chelators or polyethylene glycol (PEG) chains (5, 6).

The concept of multimerization has been developed to address the question of multimeric binding by "poly-potent" ligands. Multimers are formed by bridging monomeric units through linker(s) (2, 7). The multimer effect has been demonstrated in different studies, showing that the binding affinity of RGD peptides increases in the order of monomer < dimer < tetramer < octamer. For example, the cyclo(-RGDfE-)-monomer, dimer, and tetramer containing heptaethylene glycol spacer units have been shown to exhibit α_v_β_3_-binding affinities that increase by a factor of ten with each duplication of binding units (8). The integrin affinity of the DOTA-RGD octamer has been shown to be three-fold higher than that of the DOTA-RGD tetramer (7).

Recently, investigators from Purdue University suggested a concept of "bivalency" for the α_v_β_3_-binding affinity of RGD-containing peptides (1, 6, 9). The main point of this concept is that the multimeric cyclic RGD peptides are likely bivalent rather than multivalent in binding to integrin α_v_β_3_, and enough distance between two RGD motifs is the key for bivalency (1, 5, 10). For example, the dimeric peptide E[c(RGDfK)]_2_ (RGD_2_) is monovalent, whereas the dimeric peptides PEG_4_-E[PEG_4_-c(RGDfK)]_2_ (3P-RGD_2_) and G_3_-E[G_3_-c(RGDfK)]_2_ (3G-RGD_2_) (G = G_3_ = Gly-Gly-Gly linker) are bivalent because of the increased distance between the two cyclic RGD motifs for simultaneous integrin α_v_β_3_ binding in the latter two peptides (5). The cyclic RGD tetramers, such as DOTA-RGD_4_ and DOTA-E{G_3_-E[G_3_-c(RGDfK)]_2_}_2_ (DOTA-6G-RGD_4_), are also likely bivalent in binding to integrin α_v_β_3_ even though they contain four identical RGD motifs (5, 10). Studies with three other tetramers (DOTA-2P-RGD_4_, DOTA-2P4G-RGD_4_, and DOTA-6P-RGD_4_) have further shown that the three tetramers are not tetravalent, although the tetramers exhibited a higher binding affinity to α_v_β_3_ than monomers and dimers, and the "locally enriched" RGD concentration has been considered to contribute to the higher binding affinity (1, 6). The linkers between RGD motifs may have a significant impact on the integrin α_v_β_3_-targeting capability, biodistribution, excretion kinetics, and metabolic stability of cyclic RGD peptides (1, 11, 12).

This chapter summarizes the data obtained with ^111^In(DOTA-6P-RGD_4_). Other chapters summarize the data obtained with ^111^In(DOTA-2P-RGD_4_) and ^111^In(DOTA-2P4G-RGD_4_), respectively.

### Related Resource Links:

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=integrin%20%CE%B1v%CE%B23) and protein (http://www.ncbi.nlm.nih.gov/protein?term=integrin%20%CE%B1v%CE%B23) sequences of integrin α_v_β_3_

Integrin α_v_β_3_-related imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=integrin+%CE%B1v%CE%B23+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Articles on integrin α_v_β_3_ (http://www.ncbi.nlm.nih.gov/omim?term=integrin%20%CE%B1v%CE%B23) in Online Mendelian Inheritance in Man

Integrin α_v_β_3_-related clinical trials (http://clinicaltrials.gov/ct2/results?term=integrin+%CE%B1v%CE%B23) in ClinicTrial.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%2021850213)]

The RGD-containing peptides were all custom-made, including P-RGD, P2G-RGD_2_, 3P-RGD_2_, and 3P-RGK_2_ (RGK = cyclo(Arg-Gly-Lys-D-Phe-Asp)). The tetramers were synthesized by the reaction of Boc-E(OSu)_2_ and their corresponding dimers (1). Conjugation of the RGD peptides with DOTA-OSu resulted in their corresponding conjugates (DOTA-P-RGD, DOTA-P-RGD_2_, DOTA-3P-RGD_2_, DOTA-2P-RGD_4_, DOTA-2P4G-RGD_4_, and DOTA-6P-RGD_4_, respectively). DOTA-6P-RGK_4_ was prepared using a procedure identical to that for DOTA-6P-RGD_4_. DOTA-6P-RGK_4_ has the identical amino acids, but its sequence is scrambled to demonstrate the RGD-specificity of DOTA-6P-RGD_4_. The identities for all RGD conjugates were confirmed, and their purities were all >95% before being used for ^111^In labeling and determination of their integrin α_v_β_3_ binding affinity. Table 1 lists the molecular weights and yields of each DOTA-conjugated peptide (1).

Table 1: The physicochemical characteristics of the RGD peptides.

Agents | DOTA-P-RGD | DOTA-P-RGD_2_ | DOTA-3P-RGD_2_* | DOTA-2P-RGD_4_ | DOTA-2P4G-RGD_4_ | DOTA-6P-RGD_4_ | DOTA-6P-RGK_4_
MW | 1,237.58 | 1,951.5 | 2,447.35 | 3,626.4 | 4,315.4 | 4,622.7 | 4,622.7
Yield | ~40% | ~41% | ~30% | ~56% | ~64% | ~43% | ~68%

*The data for DOTA-3P-RGD_2_ were obtained from Shi et al. (5).

All ^111^In-labeled peptides were prepared by reacting ^111^InCl_3_ with the respective DOTA conjugates in NH_4_OAc buffer (100 mM, pH = 5.5). Radiolabeling was completed by heating the reaction mixture at 100°C for ~15 min. After purification, the radiochemical purity was >95% and the specific activity was >40 mCi/μmol (1.48 GBq/µmol) for all ^111^In-labeled RGD peptides (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%2021850213)]

The integrin binding affinity and specificity of the RGD peptides were assessed in U87MG human glioma whole cells, with ^125^I-c(RGDyK) as the integrin-specific radioligand (1). The α_v_β_3_ binding affinity of the peptides followed the order of DOTA-6P-RGD_4_ ~ DOTA-2P4G-RGD_4_ ~ DOTA-2P-RGD_4_ > DOTA-P-RGD_2_ > DOTA-P-RGD > RGD (IC_50_ = 49.9) (Table 1). The binding affinity of DOTA-3P-RGD_2_ was significantly higher than that of DOTA-P-RGD and DOTA-P-RGD_2_ (P < 0.01). However, the investigators found that the integrin α_v_β_3_ binding affinities of DOTA-2P-RGD_4_, DOTA-2P4G-RGD_4_, and DOTA-6P-RGD_4_ were only marginally higher than that of DOTA-3P-RGD_2_, suggesting that they might share the same bivalency in binding to the integrin α_v_β_3_.

Shi et al. also determined the water-octanol partition coefficients and stability of the ^111^In-labeled peptides (1). The log P values are listed in Table 2. The ^111^In-labeled peptides remained stable for >72 h after purification in the presence of 3 mM EDTA.

Table 2: The IC_50_ and log P values of the ^111^In-labeled cyclic RGD peptides.

Peptides | DOTA-P-RGD | DOTA-P-RGD_2_ | DOTA-3P-RGD_2_ | DOTA-2P-RGD_4_ | DOTA-2P4G-RGD_4_ | DOTA-6P-RGD_4_ | DOTA-6P-RGK_4_
IC_50_ (nM) | 44.3 | 5.0 | 1.5 | 0.5 | 0.2 | 0.3 | 437
Log P | -3.48 | -3.22 | -4.20 | -3.87 | -3.93 | -3.68 | -3.61

IC_50_: half-maximal inhibitory concentration.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%2021850213)]

Biodistribution, imaging, and metabolic studies were performed in athymic nude mice bearing U87MG human glioma xenografts in both left and right upper flanks (1).

For the biodistribution studies, each mouse was administered ~3 μCi (~0.111 MBq) of the agent via tail vein injection (1). Mice were then euthanized at 0.5, 1, 4, 24, and 72 h after injection (n = 5 mice/time point). The organ uptake was calculated as the percentage of injected dose per gram of organ mass (% ID/g). ^111^In(DOTA-6P-RGD_4_) was excreted mainly via the renal route, with >75% of the injected radioactivity recovered from urine and <10% of the injected radioactivity from feces. ^111^In(DOTA-6P-RGD_4_) had a rapid blood clearance, with high tumor/blood ratios. In the tumor, the agent had a high initial uptake (10.5% ID/g at 0.5 h after injection), with a slow radioactivity washout (half maximal radioactivity = ~40 h). In the liver, ^111^In(DOTA-6P-RGD_4_) had a moderately low uptake and high tumor/liver ratios. However, ^111^In(DOTA-6P-RGD_4_) had significant uptake in the kidneys and intestine (Table 3).

Table 3: Selected biodistribution data of ^111^In(DOTA-6P-RGD_4_).

% ID/g | 0.5 h | 1 h | 24 h | 72 h
Blood | 0.92 ± 0.06 | 0.29 ± 0.14 | 0.12 ± 0.02 | 0.06 ± 0.00
Kidney | 10.68 ± 1.79 | 7.21 ± 0.79 | 4.27 ± 0.22 | 3.10 ± 0.38
Liver | 4.09 ± 0.54 | 4.01 ± 0.41 | 1.50 ± 0.17 | 1.23 ± 0.27
U87MG | 10.48 ± 1.83 | 11.08 ± 2.38 | 6.86 ± 1.87 | 3.04 ± 0.39
Tumor/Blood | 11.32 ± 1.71 | 46.41 ± 25.60 | 56.45 ± 10.80 | 52.90 ± 4.95
Tumor/Kidney | 0.99 ± 0.19 | 1.56 ± 0.41 | 1.60 ± 0.39 | 1.00 ± 0.21
Tumor/Liver | 2.55 ± 0.21 | 2.79 ± 0.73 | 3.24 ± 1.02 | 2.60 ± 0.80
Tumor/Lungs | 2.61 ± 0.33 | 3.13 ± 1.09 | 4.68 ± 1.72 | 4.70 ± 0.86
Tumor/Muscle | 5.83 ± 0.80 | 10.90 ± 2.51 | 13.09 ± 2.85 | 13.47 ± 3.64

For the blocking experiment, each mouse was administered ~3 μCi (~0.111 MBq) ^111^In(DOTA-6P-RGD_4_) along with ~350 μg (~14 mg/kg) RGD_2_ (n = 5 mice) (1). Animals were euthanized at 1 h after injection. Co-injection of excess RGD_2_ significantly blocked the tumor uptake of ^111^In(DOTA-6P-RGD_4_) (0.7% ID/g with RGD_2_versus 11.1% ID/g without RGD_2_). The normal organ uptake of ^111^In(DOTA-6P-RGD_4_) was also blocked by the presence of excess RGD_2_. The uptake values of ^111^In(DOTA-6P-RGD_4_) without excess RGD_2_ in the eyes, heart, intestine, liver, lungs, and spleen were 1.4, 0.8, 11.5, 4.0, 3.7, and 2.1% ID/g, respectively, while its uptake values with excess RGD_2_ in the same organs were 0.1, 0.4, 0.5, 0.7, 1.2, and 0.5% ID/g, respectively (1).

To study the RGD specificity, comparative analysis was performed for tumor uptake values of ^111^In(DOTA-6P-RGD_4_) and control ^111^In(DOTA-6P-RGK_4_) at 60 min after injection (1). The control tetramer ^111^In(DOTA-6P-RGK_4_) had much lower tumor uptake values (0.8% ID/g) than those of ^111^In(DOTA-6P-RGD_4_) (11.1% ID/g) (P < 0.01). ^111^In(DOTA-6P-RGK_4_) also had significantly lower uptake values than those of ^111^In(DOTA-6P-RGD_4_) in the normal organs, such as intestine, kidneys, liver, lungs, and spleen (P < 0.01). These results indicate that replacing the RGD motifs with RGK will result in a dramatic uptake decrease in the tumor and α_v_β_3_-positive organs, particularly the intestine, liver, lungs, and spleen.

The imaging studies were performed after tail vein administration of ~100 μCi (3.7 MBq) ^111^In(DOTA-6P-RGD_4_) (n = 3 mice) (1). The whole-body images were acquired at 0.5, 1, 4, 24, and 72 h after injection. The tumors were clearly visualized with excellent tumor/background contrast as early as 1 h after injection. A long tumor retention time was observed, which was consistent with the biodistribution results. The time to half-maximal radioactivity in tumors was >30 h for ^111^In(DOTA-2P-RGD_4_), ^111^In(DOTA-2P4G-RGD_4_), and ^111^In(DOTA-6P-RGD_4_) (1).

For the metabolism studies, each mouse was given ~100 μCi (3.7 MBq) ^111^In(DOTA-6P-RGD_4_) via tail vein injection (1). The urine samples were collected at 30 min and 120 min after injection, and the feces samples were collected at 120 min after injection. The percentage of radioactivity recovery was >95% (by γ-counting) for both urine and feces. There was very limited radioactivity accumulation in the liver and kidneys. ^111^In(DOTA-6P-RGD_4_) maintained its integrity during its excretion via the renal route; however, there was a significant metabolism during its excretion via the hepatobiliary route, with only ~45% of intact ^111^In(DOTA-6P-RGD_4_) in the feces sample.

Shi et al. comparatively analyzed the biodistribution data for ^111^In(DOTA-2P-RGD_4_), ^111^In(DOTA-2P4G-RGD_4_), ^111^In(DOTA-6P-RGD_4_), ^111^In(DOTA-6G-RGD_4_), ^111^In(DOTA-3P-RGD_2_), ^111^In(DOTA-P-RGD_2_), and ^111^In(DOTA-P-RGD) (1). Over the first 24 h, the tumor uptake difference between the tetramers and dimers was not significant (P > 0.05). The tumor uptake at 72 h (% ID/g) followed the general order of ^111^In(DOTA-6P-RGD_4_) (3.04) > ^111^In(DOTA-2P-RGD_4_) (2.87) ~ ^111^In(DOTA-2P4G-RGD_4_) (2.66) > ^111^In(DOTA-3P-RGD_2_) (2.18), which was similar to the trend observed with integrin α_v_β_3_ binding affinity (IC_50_, nM) of DOTA-6P-RGD_4_ (0.3 ± 0.1) ~ DOTA-2P4G-RGD_4_ (0.2 ± 0.1) ~ DOTA-2P-RGD_4_ (0.5 ± 0.1) > DOTA-3P-RGD_2_ (1.5 ± 0.2). Among the ^111^In-labeled radiotracers, ^111^In(DOTA-6G-RGD_4_) had the highest uptake in the tumor and intestine at 72 h after injection. The half-life of ^111^In(DOTA-6G-RGD_4_) in the tumor was estimated to be 60 h. In contrast, ^111^In(DOTA-3P-RGD_2_) and ^111^In(DOTA-2P4G-RGD_4_) had low uptake in the intestine, kidneys, and liver over the 72-h period. As a result, ^111^In(DOTA-3P-RGD_2_) and ^111^In(DOTA-2P4G-RGD_4_) had tumor/kidney and tumor/liver ratios that were significantly better (P < 0.05) than those of ^111^In(DOTA-6G-RGD_4_) and ^111^In(DOTA-6P-RGD_4_) during that period of time. As expected, ^111^In(DOTA-P-RGD) had the lowest tumor uptake (3.7% ID/g and 0.7% ID/g at 0.5 h and 72 h after injection, respectively). ^111^In(DOTA-P-RGD_2_) had a relatively high tumor uptake (6.1 at 0.5 h after injection), but it had a significant washout from the tumor, with uptake values being 4.9, 4.8, 3.1, and 1.6% ID/g at 1, 4, 24, and 72 h after injection, respectively. The tumor uptake values follow the trend of ^111^In(DOTA-3P-RGD_2_) > ^111^In(DOTA-P-RGD_2_) > ^111^In(DOTA-P-RGD), which was consistent with the order of their α_v_β_3_ binding affinities (IC_50_ value): DOTA-3P-RGD_2_ < DOTA-P-RGD_2_ < DOTA-P-RGD.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed)]

No references are currently available.

## References

1 Shi J., et al. (2011). Evaluation of In-Labeled Cyclic RGD Peptides: Effects of Peptide and Linker Multiplicity on Their Tumor Uptake, Excretion Kinetics and Metabolic Stability. Theranostics.
2 Dijkgraaf I., Beer A.J., Wester H.J. (2009). Application of RGD-containing peptides as imaging probes for alphavbeta3 expression. Front Biosci.
3 Gaertner, F.C., M. Schwaiger, and A.J. Beer, Molecular imaging of avb3 expression in cancer patients. Q J Nucl Med Mol Imaging, 2010
4 Lu, X. and R.F. Wang, A Concise Review of Current Radiopharmaceuticals in Tumor Angiogenesis Imaging. Curr Pharm Des, 2012
5 Shi J., et al. (2011). Impact of bifunctional chelators on biological properties of 111In-labeled cyclic peptide RGD dimers. Amino Acids.
6 Liu S. (2009). Radiolabeled cyclic RGD peptides as integrin alpha(v)beta(3)-targeted radiotracers: maximizing binding affinity via bivalency. Bioconjug Chem.
7 Li Z.B., et al. (2007). (64)Cu-labeled tetrameric and octameric RGD peptides for small-animal PET of tumor alpha(v)beta(3) integrin expression. J Nucl Med.
8 Poethko T., et al. (2004). Chemoselective pre-conjugate radiohalogenation of unpretected mono- and multimeric peptides via oxime formation. Radiochim Acta.
9 Chakraborty S., et al. (2010). Evaluation of 111In-labeled cyclic RGD peptides: tetrameric not tetravalent. Bioconjug Chem.
10 Shi J., et al. (2009). Improving tumor uptake and pharmacokinetics of (64)Cu-labeled cyclic RGD peptide dimers with Gly(3) and PEG(4) linkers. Bioconjug Chem.
11 Liu Z., et al. (2009). (68)Ga-labeled cyclic RGD dimers with Gly3 and PEG4 linkers: promising agents for tumor integrin alphavbeta3 PET imaging. Eur J Nucl Med Mol Imaging.
12 Shi J., et al. (2008). Improving tumor uptake and excretion kinetics of 99mTc-labeled cyclic arginine-glycine-aspartic (RGD) dimers with triglycine linkers. J Med Chem.